# Pyro-Gly-Asp-Glu-Val-Asp-Gly-Ser-Gly-Lys(BHQ3)

Chemical name: | Pyro-Gly-Asp-Glu-Val-Asp-Gly-Ser-Gly-Lys(BHQ3)
Abbreviated name: | PPB
Synonym:
Agent category: | Peptide
Target: | Caspase-3
Target category: | Enzyme
Method of detection: | Optical imaging, near-infrared (NIR) fluorescence
Source of signal/contrast: | Pyropheophorbide α (Pyro)
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PPB)]

Photodynamic therapy (PDT), also known as photochemotherapy, uses light-activated photosensitizers (PS) in the presence of oxygen to kill cells (1). PDT has become a promising modality to treat skin, esophagus, and lung cancers, as well as other diseases such as atherosclerosis, macular degeneration, and rheumatoid arthritis (2). In PDT, light excites the singlet state of the PS, followed by intersystem transition from the singlet state to the triplet state; then, the energy is transferred from the triplet state of the PS to the triplet ground state of oxygen ^3^O_2_(X^3^Σ_g_^-^) (^3^O_2_ triplet state quenching) to generate singlet oxygen ^1^O_2_(a^1^Δ_g_) (3). The produced ^1^O_2_ is a major cytotoxic agent that has a short life time (<200 ns) and an average diffusion range (~20 nm, which is smaller than the diameter of a cell) (2). Such a short diffusion range requires the delivery of target-specific PS agents into subcellular compartments such as cytoskeletal tubulin, lysosomes, mitochondria, plasma membrane, and the nucleus, where they can generate ^1^O_2_ efficiently (2). A novel type of PS agents, called a photodynamic molecular beacon (PMB) or killer beacon, has been developed to meet this requirement (2, 4). A typical PMB consists of four modular components: a fluorescent PS, a quencher, a linker, and a delivery vehicle. The target-specific linkers keep the fluorescent PS and the quencher within the effective distance of the Föster radius (3–6 nm) (2), which allows efficient fluorescence resonance energy transfer between the fluorescent PS and the quencher. As a result, the fluorescent PS is silent until the PMB meets the target, where the enzyme cleaves the linker and activates the fluorescence of the PS (4). Thus, the PS performs two functions by producing ^1^O_2_ to kill cells and by illuminating detectable fluorescence to image its own therapeutic outcome (5).

Caspases are cysteine aspartate proteinases (6), and they participate in apoptosis through direct disassembly of cell structure, cleavage of several important proteins (gelsolin, focal adhesion kinase, and p21), shutting down DNA replication and repair, disrupting nuclear structure, and disintegrating cells into apoptotic bodies (7). As a main downstream effector, the caspase subtype-3 (capspase-3) recognizes targets that contain the tetrapeptide sequence Asp-Glu-Val-Asp (7). Proteins with this recognition motif are cleaved specifically with high efficiency (k_cat_/K_m_ > 10^6^ M^-1^s^-1^). Pyro-Gly-Asp-Glu-Val-Asp-Gly-Ser-Gly-Lys(BHQ3) (PPB) is a PMB specific for caspase-3, and it is detectable with near-infrared (NIR) fluorescence imaging (5). PPB consists of the infrared fluorescence PS pyropheophorbide α (Pyro), a black hole quencher 3 (BHQ3), and a peptide linker (GDEVDGSGK) (5). The peptide contains the tetrapeptide motif DEVD for caspase-3 recognition, and the cleavage site is located between the D and G residues. Pyro acts as the intracellular vehicle and as the PS (absorption, 665 nm; emission, 675 nm and 720 nm) with good ^1^O_2_ production (50%). Pyro lacks dark toxicity (toxicity in absence of ligh) because of its low absorption between 450–600 nm. BHQ3 (absorption, 672 nm) can efficiently quench Pyro fluorescence via fluorescence resonance energy transfer (FRET). The cleavage of PPB by caspase-3 separates the photosensitizer (Pyro) from the quencher (BHQ3) and restores the Pyro fluorescence for detection.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( PPB)+AND+synthesis%0D%0A)]

Stefflova et al. reported the detailed synthesis of PPB (5). A peptide of Fmoc-GD(Boc)E(Boc)VD(Boc)GS(Boc)GK(Mtt)-Sieber resin (Boc is t-butoxycarbonyl; Mtt is methyltrityl) was synthesized by the manual, Fmoc, solid-phase, peptide synthesis protocol with commercially available N-α-protected amino acids as building blocks, Sieber amide resin as a solid support, and N-hydroxybenzotriazole (HOBt)/2-(benzotriazole-1-yl)-1,1,3,3-tetramethyluronium hexafluorophosphate (HBTU) as amino acid activators. After the last Fmoc group cleavage, Pyro-acid was coupled to the α-NH_2_ group of N-terminal glycine of the peptide-resin at a molar ratio of 3:1. The produced peptide resin was treated with 50% trifluoroacetic acid and 5% triisopropylsilane in dichloromethane to yield Pyro-GDEVDGSGK, followed by coupling of the ε-NH_2_ of the C-terminal lysine with BHQ3-NHS to yield PPB. The product was purified with high-performance liquid chromatography and the structure was characterized by UV-vis spectroscopy and matrix-assisted laser desorption/ionization (MALDI)-time of flight mass spectrometry (TOF).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( PPB)+AND+%22in+vitro%22)]

The specificity of PPB to caspapse-3 was tested in aqueous solution (5). High-performance liquid chromatography was used to examine the cleavage product. PPB (6.3 μM) was cleaved to two pieces after incubation for 50 min with caspase-3 (0.2 μg). An immediate increase of fluorescence was observed, which reached a plateau at 90 min with as much as an 8-fold increase. This increase was not observed for PPB alone, for the presence of PPB (6.3 μM) with caspase-3 inhibitor (Ac-DEVD-CHO, 100 μM), or the presence of scrambled PPB (Pyro-GPLGLAREK-(BHQ3) with caspase-3 (molar ratio of 200:1). Cleavage was prohibited in the presence of caspase-3–specific inhibitor or scrambled PPB, confirming that PPB was specifically cleaved by caspase-3 in solution.

Stefflova et al. used PPB to study capspase-3–triggered PDT in tumor cells in vitro (5). Hepatoblastoma G_2_ cells (HepG_2_) were incubated with 200 μM PPB for 30 min or 24 h and subsequently treated with a light dose of 5 J/cm^2^ at 670 nm. The cleavage of PPB in the cells was monitored with confocal microscopy. The PDT-treated cells exhibited a significant increase of fluorescence intensity. In comparisons, a minimal fluorescence increase was observed for the control cells that were incubated with PPB for 24 h but not exposed to the light, and the cells that were incubated with the scrambled sequence Pyro-GHSSK(BHQ3)LQL followed by exposure to light. These results demonstrate that the peptide linker in the PPB was cleaved within the PDT-treated cells, which induced significant increases in the Pyro fluorescence. To further confirm that this cleavage is apoptosis-related, Apoptag, a terminal [underlined: deoxynucleotidyl] (http://en.wikipedia.org/wiki/Nucleotide) transferase–mediated dUTP nick end labeling (TUNEL) assay, was used to examine apoptosis-related DNA cleavage in the HepG_2_ cells that were incubated with PPB and treated with PDT. The fluorescence from Pyro (633 nm) as a result of the caspase-3–dependent cleavage of PPB and the fluorescence from fluorescein (488 nm) as a result of Apoptag stain were found in the same cellular compartment, which confirmed that apoptosis induced PPB cleavage in vitro.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( PPB) +AND++rodentia)]

Stefflova et al. studied the cleavage of PPB in vivo with fluorescent imaging (5). Nude mice were subcutaneously inoculated on the upper side of the leg with 10^7^ HepG_2_ cells, and the tumor was grown for about 20 days. Immediately after subcutaneous injection of 80 nmol PPB into the tumor sites, one mouse received PDT treatment at a light dose of 150 J/cm^2^ for the whole tumor area, and the images were collected at 2, 3, and 4 h. Compared with the tumor that was injected with PPB but not treated with PDT, a visible fluorescence increase was found in the tumor treated with PPB followed by PDT treatment.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( PPB) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( PPB) +AND+human)]

No publication is currently available.

### NIH Support

CA 105008

## References

1 Dougherty T.J., Gomer C.J., Henderson B.W., Jori G., Kessel D., Korbelik M., Moan J., Peng Q. (1998). Photodynamic therapy. J Natl Cancer Inst.
2 Stefflova K., Chen J., Zheng G. (2007). Killer beacons for combined cancer imaging and therapy. Curr Med Chem.
3 Clo E., Snyder J.W., Voigt N.V., Ogilby P.R., Gothelf K.V. (2006). DNA-programmed control of photosensitized singlet oxygen production. J Am Chem Soc.
4 Zheng G., Chen J., Stefflova K., Jarvi M., Li H., Wilson B.C. (2007). Photodynamic molecular beacon as an activatable photosensitizer based on protease-controlled singlet oxygen quenching and activation. Proc Natl Acad Sci U S A.
5 Stefflova K., Chen J., Marotta D., Li H., Zheng G. (2006). Photodynamic therapy agent with a built-in apoptosis sensor for evaluating its own therapeutic outcome in situ. J Med Chem.
6 Kumar S., Richards-Kortum R. (2006). Optical molecular imaging agents for cancer diagnostics and therapeutics. Nanomed.
7 Thornberry N.A., Lazebnik Y. (1998). Caspases: enemies within. Science.